# ^99m^Tc-Labeled anti-receptor for advanced glycation endproducts monoclonal antibody F(ab’)_2_ fragments

Chemical name: | ^99m^Tc-Labeled anti-receptor for advanced glycation endproducts monoclonal antibody F(ab’)_2_ fragments | [image]
Abbreviated name: | ^99m^Tc-anti-RAGE mF(ab’)_2_ | [image]
Synonym: | ^99m^Tc-anti-RAGE F(ab’)_2_ | [image]
Agent Category: | Antibodies | [image]
Target: | Receptor for advanced glycation endproducts (RAGE) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of RAGE.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=AGE+and+RAGE)]

The ^99m^Tc-labeled anti-receptor for advanced glycation endproducts (RAGE) monoclonal antibody F(ab’)_2_ fragment, abbreviated as ^99m^Tc-anti-RAGE mF(ab’)_2_ or ^99m^Tc-anti-RAGE F(ab’)_2_, is a radiotracer developed by Tekabe et al. for imaging atherosclerotic lesions by targeting highly expressed RAGE with single-photon emission computed tomography (SPECT) (1). RAGE is a 35-kDa transmembrane receptor of the immunoglobulin (Ig) superfamily (2, 3).

RAGE has one V domain, two C domains, one transmembrane domain, and one cytoplasmic tail. The V domain consists of two N-glycosylation sites and is responsible for extracellular ligand binding. RAGE exists in three forms: full-length, membrane-bound, and soluble (2-4). Under physiological conditions, RAGE is expressed at low levels in a variety of cells in a regulated manner, but RAGE is highly expressed in a series of age- and diabetes-related chronic inflammatory diseases and cancer (5-8). The advanced glycation endproducts (AGEs) are the major ligands for RAGE. AGEs are a heterogeneous group of peptides and proteins derived from non-enzymatic glycosylation processes (3, 5). Large amounts of AGEs is formed through metabolism and aging, and this establishes a positive feedback cycle under pathological conditions such as diabetes (2, 4, 9). The interaction between AGEs and RAGE affects almost all types of cells and molecules and results in pro-inflammatory gene activation (8, 10). The pathological effects induced by the AGEs/RAGE interaction include increasing vascular permeability, inhibiting vascular dilation, inducing cytokine secretion, enhancing oxidative stress, and modulating cell response to exogenous growth factors. Understanding of the AGEs/RAGE interaction is crucial to develop new treatment regimens for age- and diabetes-related conditions and cancer (4, 10).

In the case of atherosclerosis, AGEs are formed in both diabetic and nondiabetic conditions, but to a greater extent in diabetes. RAGE itself is expressed in nearly all cell types pertinent for the development and progression of atherosclerotic plaque. The AGEs/RAGE interaction leads to diabetic vascular complications and augments atherosclerotic plaque development and progression (8, 9). In a proof-of-concept study of whether the expression level of RAGE could be detected and thus used as a marker of atherosclerosis, Tekabe et al. developed a ^99m^Tc-labeled polyclonal antibody F(ab’)_2_ fragment against RAGE and further demonstrated that uptake of the fragment in the atherosclerotic plaques could be visualized with planar γ imaging in a nondiabetic apolipoprotein E–null (ApoE^–/–^) mouse model (2). To reduce the nonspecific binding associated with the polyclonal antibody, Tekabe et al. developed a monoclonal antibody against the extracellular domain of RAGE (1). The intact monoclonal antibody was then digested with pepsin, and the generated F(ab’)_2_ fragment was radiolabeled to produce the radiotracer ^99m^Tc-anti-RAGE mF(ab’)_2_. SPECT imaging showed that the radiotracer identified early accelerated lesions in diabetic ApoE^–/–^ mice to a better degree than in nondiabetic mice. The results indicated that SPECT with ^99m^Tc-anti-RAGE mF(ab’)_2_ may be used to assess novel therapies in experimental animals and possibly in humans (1).

### Related Resource Links:

- Gene information of RAGE in GenBank (http://www.ncbi.nlm.nih.gov/gene/177)
- Article on RAGE in OMIM (http://www.ncbi.nlm.nih.gov/omim/600214)
- AGE substance in PubChem (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?sid=53787607&loc=es_rss)
- MICAD chapter on ^99m^Tc-anti-RAGE pF(ab’)_2_ (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Tekabe et al. described in detail the production and radiolabeling of the monoclonal F(ab’)_2_ fragment (1). Briefly, the peptide Ac-NRRGKEVKSNYRVRVYQIC-amide on the basis of the V domain of RAGE was synthesized and conjugated to the carrier molecule keyhole limpet hemocyanin (1, 2). After immunization of the BALB/c mice (n = 15) with the conjugated peptide, hybridomas were selected, and monoclonal antibodies were then produced in vitro (<3 endotoxin U/mg purified antibody). The F(ab')_2_ fragments were generated with pepsin digestion of the intact antibody. ^99m^Tc-Labeling of the fragments was performed with diethylenetriamine pentaacetic acid (DTPA) modification, followed by reaction with ^99m^TcO_4_- in SnCl_2_ in 0.1 N HCl. The specific activity of the ^99m^Tc-anti-RAGE mF(ab’)_2_ was 6.58 ± 0.68 MBq/µg (0.178 ± 0.018 mCi/µg) protein, and the radiochemical purity was 98 ± 0.54%. The molecular weight of the fragments and the radiolabeling yields were not reported (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Immunoreactivities of the intact antibody and antibody fragment were tested against soluble RAGE (1). The antibody concentration for the DTPA-modified F(ab')_2_ fragment and the unmodified intact antibody, given 50% of maximum binding, was 0.2 µg/ml and 0.4 µg/ml, respectively, which was equivalent to 2 × 10^-9^ mol/L or apparent affinity of 0.5 × 10^9^ L/mol for both intact antibody and antibody fragment. The results suggested no reduction of the binding capability for the DTPA-modified F(ab')_2_ fragment compared with the unmodified intact antibody.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20008983)]

Tekabe et al. measured the blood-pool clearance of ^99m^Tc-anti-RAGE mF(ab’)_2_ in C57BL/6 mice (n = 3) to determine the optimal time for imaging (1). The clearance was biexponential, with the half-life equal to 20 min for the first (fast) component and 7 h for the second (slower) component. The optimal time for imaging was 4 h after tracer injection.

For biodistribution and imaging studies, Tekabe et al. established animal models of atherosclerosis with male diabetic and nondiabetic ApoE^–/–^ mice (1). Diabetes was induced in the mice via five daily intraperitoneal injections of streptozotocin (resulting in insulin deficiency). Male ApoE^–/–^/RAGE^–/–^ mice were used as controls. Biodistribution studies were performed 5–6 h after injection of the ^99m^Tc-anti-RAGE mF(ab’)_2_, and the highest uptake was observed in the liver and spleen in both diabetic and nondiabetic ApoE^–/–^ mice (n = 6–8/group). SPECT imaging at 4 h after injection showed uptake in the atherosclerotic lesions of the proximal aorta from both diabetic and nondiabetic ApoE^–/–^ mice (n = 8/group). However, the uptake was significantly greater in the diabetic group (1.39 × 10^–2^ ± 0.16% injected dose (ID)) than in the nondiabetic group (0.48 × 10^–2^ ± 0.27% ID; P < 0.0001). The control ApoE^–/–^/RAGE^–/–^ mice (n = 6) showed no uptake of the radiotracer. The nondiabetic ApoE^–/–^ mice showed minimal uptake of the radiotracer; the significance was borderline (P = 0.05) in comparison to the ApoE^–/–^/RAGE^–/–^ mice. Atherosclerotic ApoE^–/–^ mice injected with an irrelevant ^99m^Tc-labeled antibody fragment as a control showed no tracer uptake in the atherosclerotic plaque. No blocking studies were presented. The concentration of the potential competitor, AGE, for the binding site was not determined and this topic was not considered further.

Ex vivo radioactivity counting confirmed the uptake of ^99m^Tc-anti-RAGE mF(ab’)_2_ in the proximal aortic atherosclerotic lesion, showing a close correlation for the uptakes from in vivo SPECT scans and from ex vivo counts (r = 0.82; P = 0.0001). A significant difference was also obtained for the radioactivity count between the diabetic and nondiabetic ApoE^–/–^ mice (0.36 ± 0.19% ID versus 0.052 ± 0.028% ID per gram tissue; P = 0.002). Histology of the aortic sections confirmed the formation and severity of the lesions as American Heart Association class III lesions in diabetic ApoE^–/–^ mice, class II lesions in nondiabetic ApoE^–/–^ mice, and minimal lesions in control ApoE^–/–^/RAGE^–/–^ mice.

Tekabe et al. further performed a correlative analysis between radiotracer uptake and RAGE expression (1). With immunohistochemical staining, the percentage of RAGE-positive cells in the proximal aortic lesions was more than two-fold higher in diabetic mice (37.7 ± 6.9%) than in nondiabetic mice (15.9 ± 4.7%; P = 0.0008). Total macrophage burden in the lesions was also significantly higher in the diabetic mice (28.2 ± 7.6%) than in the nondiabetic mice (13.4 ± 4.8%; P = 0.0004). RAGE was colocalized predominantly with macrophages. The radiotracer uptake correlated strongly with the RAGE expression (r = 0.82; P = 0.002) and with the macrophage burden (r = 0.86; P < 0.0001). The specificity of the anti-RAGE antibody was further confirmed by the lack of staining in the aortic lesions in the control ApoE^–/–^/RAGE^–/–^ mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Tekabe Y., Luma J., Einstein A.J., Sedlar M., Li Q., Schmidt A.M., Johnson L.L. (2010). A novel monoclonal antibody for RAGE-directed imaging identifies accelerated atherosclerosis in diabetes. J Nucl Med.
2 Tekabe Y., Li Q., Rosario R., Sedlar M., Majewski S., Hudson B.I., Einstein A.J., Schmidt A.M., Johnson L.L. (2008). Development of receptor for advanced glycation end products-directed imaging of atherosclerotic plaque in a murine model of spontaneous atherosclerosis. Circ Cardiovasc Imaging.
3 Yan S.F., Ramasamy R., Schmidt A.M. (2010). The RAGE axis: a fundamental mechanism signaling danger to the vulnerable vasculature. Circ Res.
4 Sourris K.C., Forbes J.M. (2009). Interactions between advanced glycation end-products (AGE) and their receptors in the development and progression of diabetic nephropathy - are these receptors valid therapeutic targets. Curr Drug Targets.
5 Daroux M., Prevost G., Maillard-Lefebvre H., Gaxatte C., D'Agati V.D., Schmidt A.M., Boulanger E. (2010). Advanced glycation end-products: implications for diabetic and non-diabetic nephropathies. Diabetes Metab.
6 Abe R., Yamagishi S. (2008). AGE-RAGE system and carcinogenesis. Curr Pharm Des.
7 Fang F., Lue L.F., Yan S., Xu H., Luddy J.S., Chen D., Walker D.G., Stern D.M., Schmidt A.M., Chen J.X., Yan S.S. (2010). RAGE-dependent signaling in microglia contributes to neuroinflammation, Abeta accumulation, and impaired learning/memory in a mouse model of Alzheimer's disease. FASEB J.
8 Nienhuis H.L., Westra J., Smit A.J., Limburg P.C., Kallenberg C.G., Bijl M. (2009). AGE and their receptor RAGE in systemic autoimmune diseases: an inflammation propagating factor contributing to accelerated atherosclerosis. Autoimmunity.
9 Walcher D., Marx N. (2009). Advanced glycation end products and C-peptide-modulators in diabetic vasculopathy and atherogenesis. Semin Immunopathol.
10 Ramasamy R., Yan S.F., Schmidt A.M. (2009). RAGE: therapeutic target and biomarker of the inflammatory response--the evidence mounts. J Leukoc Biol.